# N-[2-(4-[^18^F]Fluorobenzamido)ethyl]maleimide-Cys-Z_EGFR:1907_

Chemical name: | N-[2-(4-[^18^F]Fluorobenzamido)ethyl]maleimide-Cys-Z_EGFR:1907_
Abbreviated name: | [^18^F]FBEM-Cys-Z_EGFR:1907_
Synonym:
Agent category: | Antibody, Affibody
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907)]

Epidermal growth factor (EGF) is a growth factor composed of 53 amino acids (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with poor patient prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use for anti-cancer therapies in both Europe and North America. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2, based on the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A, was constructed (17). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. The EGFR-specific Affibody Z_EGFR:1907_ (6.7 kDa) was identified to have good affinity (K_d_ = 5.4 nM) for EGFR (HER1) and was labeled with ^111^In via isothiocyanate-benzoyl-diethylenetriamine pentaacetic acid (DTPA) to form ^111^In-Bz-DTPA-Z_EGFR:1907_ (http://www.ncbi.nlm.nih.gov/books/NBK23654/) for use with single-photon emission computed tomography (18) imaging in nude mice bearing human tumors (19). To facilitate site-specific conjugation, Ac-Cys-Z_EGFR:1907_ (Cys at the N terminal) was synthesized and conjugated with 1,4,7,10-tetraazacyclododecane-1,4,7-tris-acetic acid-10-maleimidethylacetamide (maleimido-mono-amide-DOTA) to form Ac-Cys(DOTA)-Z_EGFR:1907_ (DOTA-Z_EGFR:1907_), and the product was labeled with ^64^Cu (t_1/2_, 12.7 h) to form ^64^Cu-DOTA-Z_EGFR:1907_ for positron emission tomography imaging studies in tumor-bearing mice (20). Miao et al. (21) reported the site-specific labeling of Ac-Cys-Z_EGFR:1907_ with N-[2-(4-[^18^F]fluorobenzamido)ethyl]maleimide ([^18^F]FBEM) to form [^18^F]FBEM-Cys-Z_EGFR:1907_ for use with in vivo imaging of EGFR-positive tumors.

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR+1907+synthesis)]

Ac-Cys-Z_EGFR:1907_ was prepared with an automated solid-phase peptide synthesizer (21). [^18^F]FBEM was prepared by reaction of N-succinimidyl-4-[^18^F]fluorobenzoate with amino-ethyl-maleimide in dimethyl sulfoxide for 30 min at 50°C. [^18^F]FBEM was isolated with high-performance liquid chromatography (HPLC). [^18^F]FBEM-Cys-Z_EGFR:1907_ was prepared by reaction of [^18^F]FBEM with Cys-Z_EGFR:1907_ (15 nmol) in sodium acetate buffer (pH 7) for 40 min at room temperature. [^18^F]FBEM-Cys-Z_EGFR:1907_ was purified with PD-10 column chromatography, with a radiochemical purity of >95% as measured with HPLC. The specific activity of [^18^F]FBEM-Cys-Z_EGFR:1907_ was 10 MBq/nmol (0.27 mCi/nmol) at the end of synthesis. Total synthesis and purification time was ~3 h. [^18^F]FBEM-Cys-Z_EGFR:1907_ remained >90% intact in mouse serum for 3 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20in%20vitro)]

In vitro binding specificity tests showed that binding of [^18^F]FBEM-Cys-Z_EGFR:1907_ to A431 human epidermoid carcinoma cells expressing EGFR was mediated by the receptors because saturation of receptors by incubation with non-labeled Ac-Cys-Z_EGFR:1907_ significantly decreased binding [^18^F]FBEM-Cys-Z_EGFR:1907_ (21). [^18^F]FBEM-Cys-Z_EGFR:1907_ exhibited a dissociation constant (K_d_) value of 37 ± 3 nM for the EGFR of A431 cells as measured with saturation assay at 4°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20rodentia)]

Miao et al. (21) performed ex vivo biodistribution studies of 1.9–2.6 MBq (0.05–0.07 mCi, ~0.4 nmol) [^18^F]FBEM-Cys-Z_EGFR:1907_ in nude mice (n = 3/group) bearing A431 xenografts at 3 h after injection. Tumor accumulation of radioactivity was 3.94 ± 0.39% injected dose per gram (ID/g). Kidney, liver, and blood accumulation was 3.78%, 9.28%, and 3.75% ID/g, respectively. Accumulation in most other organs was <1.6% ID/g. Co-injection of 6.9 and 77 nmol unlabeled Ac-Cys-Z_EGFR:1907_ resulted in tumor accumulation of 8.06 ± 1.44% ID/g and 0.97 ± 0.42% ID/g, respectively. The high blocking dose inhibited tumor accumulation by 75% (P < 0.05), whereas the low blocking dose enhanced tumor accumulation by 105% (P < 0.05). The high blocking dose decreased radioactivity in most normal organs except the kidney. On the other hand, the low blocking dose exhibited a slight decrease of radioactivity in most normal organs except the lung, kidney, skin, pancreas, and bone.

PET imaging analysis was performed in nude mice bearing A431 tumors at 1 h and 3 h after intravenous injection of 1.9–2.6 MBq (0.05–0.07 mCi, ~0.4 nmol) [^18^F]FBEM-Cys-Z_EGFR:1907_ with or without co-injection of 6.9 and 77 nmol unlabeled Ac-Cys-Z_EGFR:1907_ (21). With no blocking dose, the tumor was clearly visualized at 1 h and 3 h after injection. With the 6.9-nmol blocking dose, the tumor exhibited higher tumor/background contrast than with no blocking dose. With the 77-nmol blocking dose, the tumor was not visualized at 1 and 3 h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20human)]

No publication is currently available.

## NIH Support

5R01 CA119053

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Goldman E.R., O'Shaughnessy T.J., Soto C.M., Patterson C.H., Taitt C.R., Spector M.S., Charles P.T. (2004). Detection of proteins cross-linked within galactoside polyacrylate-based hydrogels by means of a quantum dot fluororeagent. Anal Bioanal Chem.
19 Tolmachev V., Friedman M., Sandstrom M., Eriksson T.L., Rosik D., Hodik M., Stahl S., Frejd F.Y., Orlova A. (2009). Affibody molecules for epidermal growth factor receptor targeting in vivo: aspects of dimerization and labeling chemistry. J Nucl Med.
20 Miao Z., Ren G., Liu H., Jiang L., Cheng Z. (2010). Small-animal PET imaging of human epidermal growth factor receptor positive tumor with a 64Cu labeled affibody protein. Bioconjug Chem.
21 Miao Z., Ren G., Liu H., Qi S., Wu S., Cheng Z. (2012). PET of EGFR Expression with an 18F-Labeled Affibody Molecule. J Nucl Med.